# ^99m^Tc-Mercaptoacetyl-Ser-Ser-Ser-Affibody Z_HER2:342_

Chemical name: | ^99m^Tc-Mercaptoacetyl-Ser-Ser-Ser-Affibody Z_HER2:342_
Abbreviated name: | ^99m^Tc-MaSSS-Z_HER2:342_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT, gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab -F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on the 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Mercaptoacetyl-Gly-Gly-Gly (MAG3) was used a chelating linker for coupling ^99m^Tc to Z_HER2:342_ Affibody (18). ^99m^Tc-MAG3-Z_HER2:342_ has been evaluated in nude mice bearing human colon adenocarcinoma tumors, resulting in high tumor/blood and tumor/muscle ratios. However, ^99m^Tc-MAG3-Z_HER2:342_ exhibited a high hepatobiliary clearance, which resulted in a high radioactivity (30% of the injected dose) in the intestines at 4 h after injection. Mercaptoacetyl-Ser-Ser-Ser (MaSSS) was used a chelating linker for coupling ^99m^Tc to Z_HER2:342_ Affibody (19) to reduce hepatobiliary clearance. ^99m^Tc-MaSSS-Z_HER2:342_ has been evaluated in nude mice bearing human SKOV-3 ovarian carcinoma tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20synthesis)]

MaSSS-Z_HER2:342_ Affibody was prepared by standard solid phase peptide synthesis. ^99m^Tc as pertechnetate was added to a solution of MaSSS-Z_HER2:342_ containing SnCl_2_ (19). The mixture was incubated for 60 min at room temperature. The labeling efficiency of ^99m^Tc incorporation was 97.0 ± 1.2% with >99% purity. ^99m^Tc-MaSSS-Z_HER2:342_ was purified by size-exclusion chromatography. Specific activities of the preparations were not reported. ^99m^Tc-MaSSS-Z_HER2:342_ was found to be stable after incubation at 37°C for 1 h in murine blood serum (>99%) or solution containing 300-fold excess cysteine (97.1%) at 37°C for 2 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20in%20vitro)]

Engfeldt et al. (19) performed binding experiments with MaSSS-Z_HER2:342_ with use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_d_ value of MaSSS-Z_HER2:342_ was calculated to be 400 pM. The K_d_ value of Z_HER2:342_ was 80 pM. Hence, the binding affinity of the synthetic Affibody molecule MaSSS-Z_HER2:342_ was 4-fold lower than the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of ^99m^Tc-MaSSS-Z_HER2:342_ to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^99m^Tc-MaSSS-Z_HER2:342_. The antigen binding capacity of ^99m^Tc-MaSSS-Z_HER2:342_ was 69.3 ± 2.5%. The cell-bound radioactivity remained 77% of the initially bound activity at 8 h and ~65% at 24 h when the cells were incubated with ^99m^Tc-MaSSS-Z_HER2:342_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20rodentia)]

Engfeldt et al. (19) performed biodistribution studies of 0.1 MBq (2.7 μCi) ^99m^Tc-MaSSS-Z_HER2:342_ in nude mice (n = 4) bearing SKOV-3 xenografts. ^99m^Tc-MaSSS-Z_HER2:342_ (0.14 nmol) was injected s.c. to each mouse. The initial tracer accumulation in the SKOV-3 tumors was 11.5 ± 0.5% injected dose per gram (ID/g) at 4 h after injection. The radioactivity level in tumors was higher than in other organs and tissues except the kidneys (33.6 ± 1.7% ID/g) at 4 h. Blood level was 0.15% ID/g. Tumor/blood and tumor/muscle ratios were ~80 and ~600, respectively. ^99m^Tc-MaSSS-Z_HER2:342_ was 83% intact in the blood at 15 min after injection. Biodistribution studies were also performed in normal NMRI mice (n = 4) without bearing any tumors at 4 h after injection. The results showed low accumulation in all organs and tissues except with high ^99m^Tc-MaSSS-Z_HER2:342_ accumulations in the kidneys (~20% ID/g) and intestines (~10% ID/g). The kidney accumulation was higher than ^99m^Tc-MAG3-Z_HER2:342_ (~7% ID/g) and the accumulation in the intestines was lower than ^99m^Tc-MAG3-Z_HER2:342_ (~30% ID/g). Single-photon emission computed tomography (SPECT) analysis was performed in nude mice (n = 3) bearing the SKOV-3 tumors after i.v. injection of 3 MBq (81 μCi) ^99m^Tc-MaSSS-Z_HER2:342_. Tumor was clearly visualized at 6 h along with the kidneys with tumor/muscle ratio of 38. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20human)]

No publication is currently available

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Engfeldt, T., A. Orlova, T. Tran, A. Bruskin, C. Widstrom, A.E. Karlstrom, and V. Tolmachev, Imaging of HER2-expressing tumours using a synthetic Affibody molecule containing the (99m)Tc-chelating mercaptoacetyl-glycyl-glycyl-glycyl (MAG3) sequence. Eur J Nucl Med Mol Imaging, 2006
19 Engfeldt T., Tran T., Orlova A., Widstrom C., Feldwisch J., Abrahmsen L., Wennborg A., Karlstrom A.E., Tolmachev V. (2007). 99mTc-chelator engineering to improve tumour targeting properties of a HER2-specific Affibody molecule. Eur J Nucl Med Mol Imaging.